# ^99m^Tc-Affibody Z_HER2:2395_-Cys

Chemical name: | ^99m^Tc-Affibody Z_HER2:2395_-Cys
Abbreviated name: | ^99m^Tc-Z_2395_-C
Synonym:
Agent category: | Antibody fragment, Affibody
Target: | Epidermal growth factor (EGF) HER2 receptor
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395)]

Epidermal growth factor (EGF) is a cytokine of 53 amino acids (6.2 kDa) and is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2. However, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_D_) of 0.1 nM (11). ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging of human breast cancer (12-16). However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab´)_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2 was constructed on the basis of the Z-domain residues (58 amino acids) from one of the IgG-binding domains of staphylococcal protein A (17). Affibody molecules exhibit high binding affinity to HER2 with K_D_ values <100 pM. Various radiolabeled Affibody molecules have been studied in terms of their ability to image HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. A cysteine molecule was introduced at the C-terminus of Affibody molecules for site-specific coupling of ^99m^Tc to Z_HER2:2395_ Affibody to form ^99m^Tc-Z_HER2:2395_-Cys (^99m^Tc-Z_2395_-C), which has been evaluated in nude mice bearing human colon adenocarcinoma tumors (18).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20synthesis)]

^99m^Tc as pertechnetate was added to a solution of Z_2395_-C containing Na/K tartrate and SnCl_2_ (18). The mixture was incubated for 40 min at 90°C. The labeling efficiency of ^99m^Tc incorporation was >97% with >98% radiochemical purity. Specific activity of the preparation was 3.5 GBq/µmol (95 mCi/µmol). ^99m^Tc-Z_2395_-C was found to be stable after incubation for 2 h at 37°C in murine plasma.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20in%20vitro)]

Ahlgren et al. (18) performed binding experiments with Z_2395_-C with the use of a Biacore sensor chip immobilized with extracellular domain of HER2 protein. The K_D_ value of Z_2395_-C was calculated to be 27 pM. The K_D_ value of Z_HER2:342_ was 22 pM. Hence, the binding affinity of Z_2395_-C was only slightly lower than the parent Affibody molecule Z_HER2:342_. In vitro binding specificity tests showed that binding of Z_2395_-C to SKOV-3 cells expressing HER2 was receptor-mediated because saturation of receptors by preincubation with non-labeled Z_HER2:342_ significantly decreased binding of ^99m^Tc-Z_2395_-C. The antigen binding capacity of ^99m^Tc-Z_2395_-C was 86%. The cell-bound radioactivity remained at 68% of the initially bound activity for up to 24 h when the cells were incubated with ^99m^Tc-Z_2395_-C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20rodentia)]

Ahlgren et al. (18) performed ex vivo biodistribution studies of ^99m^Tc-Z_2395_-C (0.1 MBq (2.7 μCi)) in nude mice bearing LS174T xenograft tumors. ^99m^Tc-Z_2395_-C (0.14 nmol) was injected intravenously into each mouse. The initial tracer accumulation in the LS174T tumors was 7.2% injected dose per gram (ID/g) at 0.5 h and remained constant at 1, 4, and 6 h after injection. The radioactivity level in tumors was higher than in other organs and tissues (the lung, liver, spleen, and intestines) except in the kidneys (~150% ID/g) at these time points. Blood levels were ~2.4% ID/g at 0.5 h and <0.1% ID/g at 1–4 h. The biodistribution was characterized by rapid clearance of radioactivity from blood and all organs and tissues (except the liver and intestines). Tumor/blood ratios were 3, 9, 88, and 129 at 0.5, 1, 4, and 6 h after injection, respectively. Preadministration of His_6_-Z_HER2:342_ (600 µg (83 nmol)) decreased tumor accumulation by >95% (P = 0.005) at 4 h after injection. Biodistribution studies were also performed in nude mice bearing SKOV-3 tumors at 4 h after injection. The results of 15% ID/g in the SKOV-3 tumors showed biodistribution patterns similar to patterns observed in the mice bearing LS174T tumors.

Single-photon emission computed tomography analysis was performed in nude mice bearing the LS174T tumors after injection of 3 MBq (81 μCi) ^99m^Tc-Z_2395_-C. The tumor was clearly visualized at 1 h and 4 h along with the kidneys. In mice pretreated with His_6_-Z_HER2:342_, the tumors could not be visualized with ^99m^Tc-Z_2395_-C.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer: signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
18 Ahlgren S., Wallberg H., Tran T.A., Widstrom C., Hjertman M., Abrahmsen L., Berndorff D., Dinkelborg L.M., Cyr J.E., Feldwisch J., Orlova A., Tolmachev V. (2009). Targeting of HER2-expressing tumors with a site-specifically 99mTc-labeled recombinant affibody molecule, ZHER2:2395, with C-terminally engineered cysteine. J Nucl Med.